# (S,S)-[^11^C]Methylreboxetine

Chemical name: | (S,S)-[^11^C]Methylreboxetine
Abbreviated name: | (S,S)-[^11^C]MRB
Synonym: | [^11^C]MeNER, [^11^C]-O-methylreboxetine, (2S, 3S)-[^11^C]MRB
Agent Category: | Compound
Target: | Brain norepinephrine transporter (NET)
Target Category: | Transporter binding
Method of detection: | PET
Source of signal: | ^11^C
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=11C-MRB%20OR%2011C-methylreboxetine)]

(S,S)-[^11^C]Methylreboxetine ((S,S)-[^11^C]MRB) is a radioligand developed for positron emission tomography (PET) imaging of the brain adrenergic receptors. It is a derivative of reboxetine, a norepinephrine transporter (NET) inhibitor, labeled with ^11^C, a positron emitter with a physical half-life (t_½_) of 20.4 min (1).

Many diseases affect the sympathetic nervous system (SNS), and imaging of pathologic changes of adrenergic transmission has been an important area of PET research (2, 3). Most postganglionic sympathetic neurons in the autonomic nervous system release the neurotransmitter norepinephrine (NE), which stimulates adrenergic receptors in various effector organs (4). There are different types and subtypes of adrenergic receptors, and they are characterized as α_1a_ to α_1c_, α_2a_ to α_2c_, and β_1_ to β_3_ (5). All of the NE receptors belong to the G-protein-linked receptor superfamily and mediate slow neuromodulatory postsynaptic responses. The NET is a transmembrane protein located in the adrenergic nerve terminals that is responsible for active reuptake (uptake-1) of NE released from neurons (6). NE is stored in the neuronal vesicles and is released on stimulation. Significant expression of NET is found in major organs of the SNS, such as the heart and brain. There is substantial evidence that aberrations in cardiac SNS function contribute to the morbidity and mortality associated with cardiac diseases (7). Brain NETs are involved in various neurologic and psychiatric diseases, including depression, attention deficit hyperactivity disorder, drug addiction, and eating disorders (8). NETs are also the site of action of many antidepressant drugs in the brain (9).

Molecular probes with structures closely related to NE can be used to assess the integrity of presynaptic sympathetic nerve terminals in various diseases. In vivo NE synthesis is similar to dopamine synthesis, and dopamine is converted to NE by the enzyme dopamine-β-hydroxylase (5). [^123^I]-meta-Iodobenzylguanidine, [^11^C]meta-hydroxyephedrine, [^11^C]norepinephrine, and many other radioligands have been developed and used for peripheral neuronal imaging (10). However, this class of tracers is not suitable for the study of brain NET system because they are not able to cross the blood-brain barrier (11). In the brain, NET levels are relatively lower than those of other receptors, such as dopamine transporters (DATs) and serotonin transporters (9). Several NET reuptake inhibitors, for example, [^11^C]desipramine, have been tested, but they showed high nonspecific binding. Reboxetine ((RS)-2-[(RS)-2-ethoxyphenoxy)benzyl]morpholine) is a specific NET inhibitor with a high affinity and selectivity (IC_50_ DAT/NET = 4,000). It has been developed in Europe for the treatment of depressive illness. Reboxetine is available as a racemic mixture of the (R,R) and (S,S) enantiomers. The (S,S) enantiomer has been found to be more potent, with a IC_50_ of 3.6 nM for inhibiting NE uptake in rat hypothalamic synaptosomes. Among the different reboxetine derivatives that have been tested, (S,S)-MRB has an IC_50_ of 2.5 nM ((R,R)-MRB has an IC_50_ of 85 nM) and is considered a promising candidate to be developed as a PET ligand for studying the brain NET system.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-MRB%20OR%2011C-methylreboxetine%29%20AND%20synthesis)]

Based on the report of Melloni et al. (12) on the synthesis and activity of reboxetine, Wilson et al. (9) first published the radiosynthesis of (S,S)-[^11^C]MRB by ^11^C methylation of the normethyl precursor, (S,S)-2-(morpholin-2-yl-phenyl-methoxy)-phenol, in a high-performance liquid chromatography (HPLC) sample loop method. [^11^C]Iodomethane was reacted with the precursor, which had been treated with methanolic tetrabutylammonium hydroxide. Radiochemical yields were 25-40% (uncorrected, based on [^11^C]iodomethane trapped), and the synthesis time was 25 min from the end of bombardment (EOB). After HPLC purification and filtration through a 0.22 μm filter, the final product was >98% radiochemically pure and >97% optically pure. The specific activity was 35-65 GBq (0.95-1.76 Ci)/μmol.

Lin and Ding (13) developed a nine-step synthetic procedure to prepare the racemic precursor, (2S,3S)/(2R,3R)-2-[α-(2-hydroxphenoxy)benzyl]-morpholine ((2S,3R)-desethylreboxetine). This procedure started with catechol monoprotected with a methanesulfonyl group. The protecting group was removed by use of excess hydride reducing agent at the end of the procedure. The racemic precursor was resolved by chiral HPLC into >98% enantiomerically pure individual precursors. Selective ^11^C O-methylation was carried out by reacting (2S, 3S)-desethylreboxetine in dimethylformamide and excess sodium hydroxide with [^11^C]methyl iodide at 100 °C for 10 min. At the end of the reaction, the product was purified by HPLC. Radiochemical yields were 61-74% (decay-corrected from [^11^C]methyl iodide), and the synthesis time was 40 min from EOB. Radiochemical purity was >96%, and the specific activity was 62.9-85.1 GBq (1.7-2.3 Ci)/μmol at EOB.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-MRB%20OR%2011C-methylreboxetine%29%20AND%20in%20vitro)]

Wilson et al. (9) measured the partition coefficient (P) of (S,S)-[^11^C]MRB and determined that the log P between 1-octanol and 0.02 M phosphate buffer at pH 7.4 was 2.35 (± 0.06; n = 12). In vitro incubation of slide-mounted rat brain coronal sections with 10 nM (S,S)-[^11^C]MRB for 10 min produced a regional distribution pattern that was similar to patterns of [^3^H]nisoxetine, an NET uptake inhibitor. High amounts of radioactivity were found in the anteroventral nucleus of the thalamus, the bed nucleus of the stria terminalis, the paraventricular nucleus of the hypothalamus, and the locus coeruleus and subcoeruleus areas. Co-incubation with 100 μM desipramine (NE reuptake inhibitor) abolished binding in all studies.

Ding et al. (11) reported that the log P of (S,S)-[^11^C]MRB was 1.17 (between octanol and 0.1 M phosphate buffer). Human plasma protein binding of (S,S)-[^11^C]MRB was determined to be 14%.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-MRB%20OR%2011C-methylreboxetine%29%20AND%20rodentia)]

Biodistribution and metabolism studies of (S,S)-[^11^C]MRB in rats were conducted by Wilson et al. (9). Each rat received (S,S)-[^11^C]MRB (8-33 MBq (0.22-0.89 mCi)/1-2 nmole) by i.v. injection. Rats were killed by decapitation at various time intervals after injection. Brain uptake was moderate (0.53% of injected dose (ID) at 5 min) with a slow washout of radioactivity in NET-rich brain regions (hypothalamus and cortex) and a faster washout in NET-poor regions (striatum). A hypothalamus/striatum ratio of 2.5 was reached at 60 min. Pretreatment of rats with reboxetine or desipramine resulted in no specific retention of radioactivity in the hypothalamus or other NET-rich regions. HPLC analysis of serum and brain samples showed that (S,S)-[^11^C]MRB was rapidly metabolized in the blood. Only 50% of (S,S)-[^11^C]MRB remained unchanged at 30 min and 20% after 60 min. In the brain, >95% of radioactivity was unchanged (S,S)-[^11^C]MRB. All radioactive metabolites were found to be hydrophilic.

Ding et al. (11) studied (S,S)-[^11^C]MRB metabolism in mice by radio-HPLC of brain tissue obtained at 10 min after injection. They determined that >95% of radioactivity was unmetabolized (S,S)-[^11^C]MRB.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-MRB%20OR%2011C-methylreboxetine%29%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-MRB%20OR%2011C-methylreboxetine%29%20AND%20%28primate%20NOT%20human%29)]

Ding et al. (11, 14) evaluated (S,S)-[^11^C]MRB as a radioligand for PET imaging studies of brain NET systems in baboons. The average specific activity at the time of injection was ~18.5-55.5 GBq (0.5-1.5 Ci)/μmol. The radiochemical purity was >98%, and enantiomeric purity was 99%. A dose of (S,S)-[^11^C]MRB (74-111 MBq (2-3mCi)) was administered i.v. to three adult female baboons. Two doses were used when a comparison or blocking study was conducted. The first dose was used for the baseline PET study, and the second dose was administered 2-3 h after the first dose for the pretreatment study with desipramine. Imaging studies showed moderate brain uptake with a peak brain uptake of 3.2-4% ID. Clearance of radioactivity in NET-rich regions (thalamus and cerebellum) was slow, whereas washout was faster in striatum and cortical regions. The t_½_ for clearance from peak uptake in the thalamus was ~250 min. The ratio of the distribution volume (DV) in the NET-rich regions to the DV in the NET-poor regions was 1.8-2.2. Pretreatment with nisoxetine (1 mg/kg) markedly reduced the uptakes by ~50% in the thalamus and ~40% in the cerebellum, but not in the striatum. This showed the saturable and specific binding of (S,S)-[^11^C]MRB to NETs in the brain. However, there was also a relatively high striatum uptake because of possible nonspecific binding. Pretreatment with desipramine also led to reduced heart radioactivity uptake. In comparison, (R,R)-[^11^C]MRB showed similar radioactivity uptakes and similar clearance kinetics in all baboon brain regions, and there was no nisoxetine blocking effect on binding. HPLC analysis of baboon plasma showed that the fractions of unchanged (S,S)-[^11^C]MRB were 98, 59, 41, 39, and 33% at 1, 5, 10, 30, and 60 min after administration, respectively. Only polar metabolites were detected in the plasma samples.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%2811C-MRB%20OR%2011C-methylreboxetine%29%20AND%20human)]

No publication is currently available.

## References

1 Rosenspire KC, Haka MS, Van Dort ME, Jewett DM, Gildersleeve DL, Schwaiger M, Wieland DM. (1990). Synthesis and preliminary evaluation of carbon-11-meta-hydroxyephedrine: a false transmitter agent for heart neuronal imaging. J Nucl Med.
2 Konishi J., Dwamena B.A., Gross M.D., Shapiro B., Misaki T., Fukunaga M., Sisson J.C., Oei H.-Y., De Jong M., Krenning E.P. Endocrinology, in Molecular Nuclear Medicine. L.E. Feinendegen, W.W. Shreeve, W.C. Eckelman, Y.-W. Bahk, and H.N. Wagner Jr., Editor. 2003, Springer: New York. p. 357-409.
3 Antoni G., Kihlberg T., Langstrom B. Aspects on the synthesis of 11C-Labelled compounds, in Handbook of Radiopharmaceuticals, M.J. Welch, and C.S. Redvanly, Editor. 2003, John Wiley & Sons Ltd.: West Sussex, England. p. 141-194.
4 Sunderland P.M. Pathophysiology. The Biologic basis for disease in adults and children, K.L. McCance, and S. E. Huether, Editor. 1994, Mosby-Year Books, Inc.: St, Louis. p. 397-436.
5 Frey K.A. PET study of neurochemical systems, in Positron Emission Tomography, P.E. Valk, D.L. Bailey, D.W. Townsend, and M.N. Maisey, Editors. 2002, Springer London. p. 309-327.
6 Buursma AR, Beerens AM, de Vries EF, van Waarde A, Rots MG, Hospers GA, Vaalburg W, Haisma HJ. (2005). The Human Norepinephrine Transporter in Combination with 11C-m-Hydroxyephedrine as a Reporter Gene/Reporter Probe for PET of Gene Therapy. J Nucl Med.
7 Caldwell JH, Kroll K, Li Z, Seymour K, Link JM, Krohn KA. (1998). Quantitation of presynaptic cardiac sympathetic function with carbon-11-meta-hydroxyephedrine. J Nucl Med.
8 Zahniser NR, Doolen S. (2001). Chronic and acute regulation of Na+/Cl- -dependent neurotransmitter transporters: drugs, substrates, presynaptic receptors, and signaling systems. Pharmacol Ther.
9 Wilson AA, Johnson DP, Mozley D, Hussey D, Ginovart N, Nobrega J, Garcia A, Meyer J, Houle S. (2003). Synthesis and in vivo evaluation of novel radiotracers for the in vivo imaging of the norepinephrine transporter. Nucl Med Biol.
10 Langer O, Halldin C. (2002). PET and SPET tracers for mapping the cardiac nervous system. Eur J Nucl Med Mol Imaging.
11 Ding YS, Lin KS, Logan J, Benveniste H, Carter P. (2005). Comparative evaluation of positron emission tomography radiotracers for imaging the norepinephrine transporter: (S,S) and (R,R) enantiomers of reboxetine analogs ([11C]methylreboxetine, 3-Cl-[11C]methylreboxetine and [18F]fluororeboxetine), (R)-[11C]nisoxetine, [11C]oxaprotiline and [11C]lortalamine. J Neurochem.
12 Melloni P, Carniel G, Della Torre A, Bonsignori A, Buonamici M, Pozzi O, Ricciardi O, Rocci AC. (1984). Potential antidepressant agents, alpha-Aryloxy-benzyl derivatives of ethanolamine and morpholine. Eur J Med Chem.
13 Lin KS, Ding YS. (2004). Synthesis, enantiomeric resolution, and selective C-11 methylation of a highly selective radioligand for imaging the norepinephrine transporter with positron emission tomography. Chirality.
14 Ding YS, Lin KS, Garza V, Carter P, Alexoff D, Logan J, Shea C, Xu Y, King P. (2003). Evaluation of a new norepinephrine transporter PET ligand in baboons, both in brain and peripheral organs. Synapse.